# [^11^C]2-(2-(Dimethylaminomethyl)phenylthio)-5-fluoromethylphenylamine

Chemical name: | [^11^C]2-(2-(Dimethylaminomethyl)phenylthio)-5-fluoromethylphenylamine
Abbreviated name: | [^11^C]AFM
Synonym:
Agent Category: | Compound
Target: | Serotonin transporter (SERT)
Target Category: | Ligand binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20AFM%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

The neurotransmitter serotonin (5-HT) plays a major role in a variety of brain functions such as appetite, sleep, and mood. Neuropsychiatric disorders, including major depression, schizophrenia, and Alzheimer’s and Parkinson’s diseases (1-3), involve a dysfunction of the brain’s serotonin system. The serotonergic neurons – present in wide areas of the brain, including the hypothalamus, thalamus, and cerebral cortex – bear a protein called “serotonin transporter” (SERT) (4).

The SERT, located on the cell bodies and terminals of 5-HT neurons, is a specific marker for the number and integrity of presynaptic terminals of serotonin-producing neurons. It regulates neurotransmission by removing released serotonin from the extracellular space back into the presynaptic neuron. Commonly prescribed antidepressants are selective serotonin reuptake inhibitors (SSRIs), and their effects are obtained through interaction with (and inhibition of) the SERT (5). For that reason, in vivo imaging of the regional brain distribution of the SERT is an important tool to study the 5-HT system and the treatment of neuropsychiatric disorders.

A variety of in vivo radioligands for positron emission tomography (PET) have been evaluated for imaging the SERT. [^11^C]McN5652 was the first successful and widely used agent (6, 7). However, it does have some limitations; for example, its kinetics in the brain are slow and its binding ratios in humans show low or nonspecificity. It is adequate for regions with high SERT density but often provides insufficient signal-to-noise differentials for imaging brain regions with intermediate to low SERT densities (e.g., limbic and neocortical regions) because of its high nonspecific binding.

Over recent years, new PET radioligands have been synthesized and evaluated as SERT imaging agents and alternatives to [^11^C]McN5652. Among them, ^11^C-labeled N,N-dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine ([^11^C]DASB), 2-(2-(dimethylaminomethyl)phenylthio)-5-fluoromethylphenylamine ([^11^C]AFM), 5-bromo-2-[2-(dimethylaminomethylphenylthio)]phenylamine ([^11^C]DAPA), 2-[2-(dimethylaminomethylphenylthio)]-5-iodophenylamine ([^11^C]ADAM), and N,N-dimethyl-2-(2´-amino-4´-hydroxymethylphenylthio)benzylamine ([^11^C]HOMADAM) (8) are based on a diaryl sulfide motif (4). [^11^C]AFM has shown high binding affinity and good selectivity for the SERT, and displays signal/noise ratios that may enable more reliable mapping of brain regions with a low density of SERT.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFA%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

AFM and its C-11 radiolabeling precursor can be prepared in a five-step procedure, as described by Huang et al. (9). Briefly, 4-chloro-3-nitrobenzyl acetate is coupled with thiosalicylic acid to give 2-(4-acetyloxymethyl-2-nitrophenylthio)benzoic acid, which is then converted to 2-(4-acetyloxymethyl-2-nitrophenylthio)-N,N-dimethylbenzamide. Reduction of the amide functionality to the tertiary amine and cleavage of the acetyl group with borane/tetrahydrofuran complex produce 2-(4-hydroxymethyl-2-nitrophenylthio)-N,N-dimethylbenzylamine. Fluorination of this compound with bis(2-methoxyethyl)aminosulfur trifluoride is then performed to produce the benzyl fluoride 2-(4-fluoromethyl-2-nitrophenylthio)-N,N-dimethylbenzylamine. Finally, reduction of the nitro group produces AFM.

Starting with 2-(4-acetyloxymethyl-2-nitrophenylthio)benzoic acid and replacing N,N-dimethylamine hydrochloride with N-methylamine hydrochloride (in the amide formation step) leads to the formation of the C-11 labeling precursor 5-fluoromethyl-2-(2-methylaminomethylphenylthio)phenylamine. [^11^C]AFM is prepared from this precursor by reaction with [^11^C]iodomethane (in dimethyl formamide, at 80-85 °C).

The chemical and radiochemical purities of [^11^C]AFM produced by this method are ≥97% (as determined by high-performance liquid chromatography). The radiochemical yield at the end of the synthesis is 12.3 ± 8.1% (decay-corrected, based on [^11^C]iodomethane; n = 14). The specific activity of the radiotracer produced is 64,121 ± 15,836 GBq/mmol (1,733 ± 428 Ci/mmol). The total synthesis time, as reported by Huang et al. (9), is about 30-37 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20AFM%20AND%20in%20vitro)]

Huang et al. (9) assayed the affinity of AFM for the SERT, norepinephrine transporter (NET), and dopamine transporter (DAT), using cloned human receptors expressed on HEK-293 cells and the radioligands [^3^H]paroxetine (for SERT), [^3^H]nisoxetine (for NET), and [^3^H]GBR12935 (for DAT). Experiments were performed according to previously published procedures (10, 11). Results showed that AFM had a high affinity and a good selectivity for SERT over NET and DAT. The authors reported the following inhibition coefficients (K_i_s): 1.04 ± 0.13, 663.8 ± 79.5, and >10,000 nM for SERT, NET, and DAT, respectively.

In comparative studies between various SERT radiotracers, Huang et al. (12) found no significant difference between the K_i_s of McN5652, ADAM, DASB, and AFM. Temperature had no significant effect on the inhibition coefficients for AFM, McN5652, and ADAM, but significantly decreased the affinity of DASB for SERT.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20AND%20AFM%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%22rodentia%22]

Biodistribution studies in Sprague-Dawley rats were performed by Huang et al. (9). The experimental procedure involved injecting 3.7 MBq (100 µCi) of [^11^C]AFM per animal (via the tail vein) and measuring the uptake of the radiotracer at 10, 30, and 60 min post injection, after sacrifice.

Results showed rapid uptake of [^11^C]AFM into the brain, with accumulation in regions rich in SERTs, such as the thalamus, hypothalamus, and cortex. The reported total brain uptakes of [^11^C]AFM at 10, 30, and 60 min post injection were 0.70, 1.06, and 1.00% of injected dose (ID)/g of tissue, respectively. The thalamus/cerebellum and hypothalamus/cerebellum activity ratios were 6.06 ± 0.17 and 6.05 ± 1.01, respectively, at 60 min post injection. When pretreated with either cold AFM (2mg/kg of tissue) or citalopram (a SSRI), the brain uptake was significantly reduced.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20AND%20AFM%20AND%20%28dog%20OR%20sheep%20OR%20pig%20OR%20rabbit%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28dog%20OR%20sheep%20OR%20pig%29]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20AFM%20AND%20%28primate%20NOT%20human%29)]

PET brain imaging studies of three adult male baboons were performed by Huang et al. (9), for time periods ranging from 0 to 90 min after administration of [^11^C]AFM. Results showed rapid distribution of the radiotracer in the brain, consistent with the regional concentrations of SERT. High uptakes were observed in the midbrain and thalamus, moderate uptakes were seen in the hippocampus and striatum, and low levels of radioactivity were detected in the cortical regions.

In all brain regions, the measured activity reached a peak followed by a substantial wash-out (e.g., maximum activity obtained at 41 ± 12 min with a wash-out of 21 ± 14% for the hippocampus). At 45 min post injection, the measured total brain uptake was 0.015 ± 0.001% ID/g of tissue, a result consistent with values obtained in rats. The reported thalamus/cerebellum, striatum/cerebellum, and hippocampus/cerebellum activity ratios were 3.3 ± 0.4, 2.4 ± 0.4, and 1.7 ± 0.3, respectively, at 90 min post injection. Significant differences in clearance were observed between the several baboons used in the study.

When the baboons were pretreated with citalopram (a SSRI; 4 and 6 mg/kg of tissue) 10 min before injection of [^11^C]AFM, a significant reduction in the brain distribution volumes was observed (30.8 ± 6.4 mL/g reduced to 15.2 mL/g (baboon A) and 29.4 ± 3.2 mL/g reduced to 21.3 mL/g (baboon B), under control conditions).

In comparative studies between the SERT radiotracers [^11^C]ADAM, [^11^C]AFM, [^11^C]DASB, [^11^C]DAPA, and [^11^C]McN5652, Huang et al. (12) showed that the regional-specific-to-nonspecific equilibrium partition coefficient was the highest for [^11^C]AFM, followed by [^11^C]DASB, [^11^C]DAPA, [^11^C]ADAM, and [^11^C]McN5652. [^11^C]AFM was shown to provide higher signal/noise ratios, which might enable more reliable measurement of SERT availability in regions of low SERT density.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20AFM%5BAll%20Fields%5D%20AND%20%28human%20NOT%20baboon%29)]

No publication is currently available.

## References

1 Owens MJ Nemeroff CB The serotonin transporter and depression Depress Anxiety 1998 8Suppl 15 12 9809208
2 Palmer AM, Francis PT, Benton JS, Sims NR, Mann DM, Neary D, Snowden JS, Bowen DM. (1987). Presynaptic serotonergic dysfunction in patients with Alzheimer's disease. J Neurochem.
3 Roth BL, Xia Z. (2004). Molecular and cellular mechanisms for the polarized sorting of serotonin receptors: relevance for genesis and treatment of psychosis. Crit Rev Neurobiol.
4 Laakso A, Hietala J. (2000). PET studies of brain monoamine transporters. Curr Pharm Des.
5 White KJ, Walline CC, Barker EL. (2005). Serotonin transporters: implications for antidepressant drug development. Aaps J.
6 Ichimiya T, Suhara T, Sudo Y, Okubo Y, Nakayama K, Nankai M, Inoue M, Yasuno F, Takano A, Maeda J, Shibuya H. (2002). Serotonin transporter binding in patients with mood disorders: a PET study with [11C](+)McN5652. Biol Psychiatry.
7 Suehiro M, Scheffel U, Ravert HT, Dannals RF, Wagner HN. (1993). [11C](+)McN5652 as a radiotracer for imaging serotonin uptake sites with PET. Life Sci.
8 Jarkas N, Votaw JR, Voll RJ, Williams L, Camp VM, Owens MJ, Purselle DC, Bremner JD, Kilts CD, Nemeroff CB, Goodman MM. (2005). Carbon-11 HOMADAM: a novel PET radiotracer for imaging serotonin transporters. Nucl Med Biol.
9 Huang Y, Hwang DR, Bae SA, Sudo Y, Guo N, Zhu Z, Narendran R, Laruelle M. (2004). A new positron emission tomography imaging agent for the serotonin transporter: synthesis, pharmacological characterization, and kinetic analysis of [11C]2-[2-(dimethylaminomethyl)phenylthio]-5-fluoromethylphenylamine ([11C]AFM). Nucl Med Biol.
10 Huang Y, Hwang DR, Zhu Z, Bae SA, Guo N, Sudo Y, Kegeles LS, Laruelle M. (2002). Synthesis and pharmacological characterization of a new PET ligand for the serotonin transporter: [11C]5-bromo-2-[2-(dimethylaminomethylphenylsulfanyl)]phenylamine ([11C]DAPA). Nucl Med Biol.
11 Laruelle M, Vanisberg MA, Maloteaux JM. (1988). Regional and subcellular localization in human brain of [3H]paroxetine binding, a marker of serotonin uptake sites. Biol Psychiatry.
12 Huang Y, Hwang DR, Narendran R, Sudo Y, Chatterjee R, Bae SA, Mawlawi O, Kegeles LS, Wilson AA, Kung HF, Laruelle M. (2002). Comparative evaluation in nonhuman primates of five PET radiotracers for imaging the serotonin transporters: [11C]McN 5652, [11C]ADAM, [11C]DASB, [11C]DAPA, and [11C]AFM. J Cereb Blood Flow Metab.